# GKVLAK–(IRIS Blue-(1,4,7,10-tetraazacyclododecane-1,4,7-tris(acetic acid t-butyl ester)-10-acetic acid monoamide))–GGGGTVQQEL

Chemical name: | GKVLAK–(IRIS Blue-(1,4,7,10-tetraazacyclododecane-1,4,7-tris(acetic acid t-butyl ester)-10-acetic acid monoamide))–GGGGTVQQEL | [image]
Abbreviated name: | DCCP16-IRIS Blue | [image]
Synonym: | | [image]
Agent Category: | Peptides | [image]
Target: | Transglutaminases | [image]
Target Category: | Enzymes | [image]
Method of detection: | Optical imaging | [image]
Source of signal / contrast: | IRIS Blue | [image]
Activation: | Yes | [image]
Studies: | - In vitro; - Rodents | Structure of DCCP16-IRIS Blue (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Transglutaminases%20and%20imaging)]

The fluorescently labeled 16-peptide agent GKVLAK-(IRIS Blue-(1,4,7,10-tetraazacyclododecane-1,4,7-tris(acetic acid t-butyl ester)-10-acetic acid monoamide (DOTAMA)))-GGGGTVQQEL, abbreviated as DCCP16-IRIS Blue, was developed by Tei et al. for optical imaging of the pathological processes associated with high transglutaminase activity (1).

Transglutaminases are a family of Ca^2+^-dependent enzymes that catalyze extracellular covalent cross-linking of proteins (2, 3). These enzymes participate in many important biological processes, such as blood coagulation, skin-barrier formation, hardening of the fertilization envelope, and extracellular matrix assembly (2, 4). They are also involved in multiple pathological processes, including wound healing, cancer, myocardial infarctions, and atherothrombosis (5-7). The fibrin-stabilizing factor XIII (FXIII, also known as plasma transglutaminase) and the tissue transglutaminase (TG2) are the two enzymes that have attracted the greatest interest in transglutaminase-targeted imaging and therapy (1, 8, 9). FXIII cross-links fibrin during blood clotting and subsequently produces a mechanically stronger clot with high fibrinolytic resistance, whereas TG2 catalyzes covalent cross-linking of the extracellular matrix. The enzyme-mediated cross-linking is achieved by forming an isopeptide bond between the γ-carbonyl group of a glutamine (Gln) in one protein and the ε-amino group of a lysine (Lys) residue in a nearby protein (3, 9). This cross-link can be blocked by covalent incorporation of an acyl-acceptor amine substrate into the fibrin units or an acyl-donor Gln-containing peptide complementary to the FXIII-reactive Lys donor cross-linking sites of the protein (1). FXIII and TG2 are much more sensitive toward the Gln-bearing substrates than to amine donor Lys residues. These transglutaminase features form the fundamental basis for the development of imaging agents for detection of transglutaminase activity. In recent years, peptides based either on β-casein and α2-antiplasmin for the Gln-donor substrate requirements or on the bovine αA-crystallin for the amine donor substrate requirements have been synthesized for in vitro transglutaminase assays, and imaging probes consisting of peptides from α2-antiplasmin have been investigated for mapping the activity of endogenous FXIII and TG2 (10-12).

Tei et al. designed a new model peptide, DCCP16, which was labeled with Gd for MRI and the fluorescent dye IRIS Blue for optical imaging (1). IRIS Blue is a cyanine dye that has an absorption maximum of 660 nm and an emission maximum of 680 nm in phosphate buffer at pH 7.4. The DCCP16 peptide consists of two moieties. The first moiety is the hexapeptide TVQQEL, which bears two Gln residues and one valine residue. The second moiety is the pentapeptide GKVLA, which is known to be a good substrate for transglutaminases. A four-glycine spacer and a Lys residue were inserted between the Lys and the Gln moieties for conjugation of the Gd-DOTAMA or the IRIS Blue-DOTAMA. This spacer-DOTAMA was chosen to keep the Gd- or IRIS Blue-complex far enough from interfering with the active site. The MRI and optical probes were therefore set as GKVLAK-(Gd-DOTAMA)-GGGGTVQQEL (Gd-DCCP16) and GKVLAK-(IRIS Blue-DOTAMA)-GGGGTVQQEL (DCCP16-IRIS Blue), respectively. In vivo effectiveness of the two agents was validated with MRI and optical mapping of transglutaminase-induced agent retention in mouse models of tumor xenografts and blood clotting (1). Noninvasive imaging of transglutaminase activity with Gd-DCCP16 or DCCP16-IRIS Blue provides an important tool for detecting and monitoring transglutaminase-targeted therapy in diverse pathologies including cancer, wound healing, myocardial infarction, and pregnancy failure associated with congenital FXIII deficiency (1). This chapter describes the results generated with DCCP16-IRIS Blue. The results obtained with Gd-DCCP16 were described in the chapter on Gd-DCCP16 in MICAD.

### Related Resource Links:

- Chapters of FXIII in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Factor%20XIII%20AND%20micad%5bbook%5d)
- Articles of transglutaminases in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/?term=Transglutaminases)
- Nucleotides (http://www.ncbi.nlm.nih.gov/nucleotide/?term=Transglutaminases) and proteins (http://www.ncbi.nlm.nih.gov/protein/?term=Transglutaminases) of transglutaminases
- Bioassays of transglutaminase activity (http://www.ncbi.nlm.nih.gov/pcassay) in PubChem BioAssay

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20812289)]

The DCCP16 peptide GKVLAKGGGGTVQQEL and the DCCP16 control GAVLAKGGGGTVAAEL were synthesized with solid-phase peptide synthesis with a rink amide resin as solid support and the standard Fmoc strategy (1). As the negative control peptide, the amino acids responsible for the transglutaminase activity of DCCP16 (Gln and Lys) were replaced with alanine. DOTAMA was coupled to the ε-NH_2_ group of the Lys residue. The purity values of both GKVLAK-(DOTAMA)-GGGGTVQQEL (DCCP16) and GAVLAK-(DOTAMA)-GGGGTVAAEL (DCCP16 control) were >95%. The yields of DCCP16 and DCCP16 control were 25% (48 mg) and 20% (35 mg), respectively. The fluorescent dye IRIS Blue was then conjugated to DCCP16 and DCCP16 control through DOTAMA. The final product DCCP16-IRIS Blue was purified and characterized. The yield of DCCP16-IRIS Blue was 16%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20812289)]

Two experiments were performed to verify that DCCP16 is covalently linked by transglutaminases (1). TG2-Mediated covalent linking between DCCP16-IRIS Blue and casein was first demonstrated by incubation of both agents in the presence of TG2 and by analysis of the product with denaturing SDS gel electrophoresis. A strong fluorescent band with a molecular weight of 25–50 kDa was observed, which corresponds to the product generated by covalent binding of more than one moiety of DCCP16-IRIS Blue (~2 kDa) to N’,N’-dimethylcasein (180 amino acids, 25–30 kDa). The results indicated that DCCP16-IRIS Blue could serve as a substrate that allows covalent cross-linking to dimethylcasein, catalyzed by TG2 (1).

TG2-Mediated covalent linking was further verified with incubation of large MCF7 (human breast cancer cell line) spheroids (1 mm in diameter) with DCCP16-IRIS Blue for 48 h (1). Strong fluorescence was observed only from spheroids treated with DCCP16-IRIS Blue.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20812289)]

Optical detection of transglutaminase activity with DCCP16-IRIS Blue was tested in animal models of thrombus (n = 6 mice) (1). Thrombi were induced on the ears of CD1 female nude mice with laser (n = 2 mice) and with thermal injury (n = 4 mice), and DCCP16-IRIS Blue was subsequently administered intravenously. During the first 20 min after administration, DCCP16-IRIS Blue distributed evenly throughout the entire tissue surrounding the wounds. After 24 h, clearance of nonbound DCCP16-IRIS Blue was complete, and bound DCCP16-IRIS Blue was seen in both wounds. After 72 h, the wounds had partly healed and the clots were partially degraded, and the fluorescence was less intense. Residual fluorescence could be detected in one of the wounds 13 days after administration. These results indicate that DCCP16-IRIS Blue could serve as an effective in vivo substrate for the detection of transglutaminase activity (1). No results were reported for DCCP16-IRIS Blue control and no blocking studies were presented.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Tei L., Mazooz G., Shellef Y., Avni R., Vandoorne K., Barge A., Kalchenko V., Dewhirst M.W., Chaabane L., Miragoli L., Longo D., Neeman M., Aime S. (2010). Novel MRI and fluorescent probes responsive to the Factor XIII transglutaminase activity. Contrast Media Mol Imaging.
2 Bergamini C.M., Griffin M., Pansini F.S. (2005). Transglutaminase and vascular biology: physiopathologic implications and perspectives for therapeutic interventions. Curr Med Chem.
3 Park D., Choi S.S., Ha K.S. (2010). Transglutaminase 2: a multi-functional protein in multiple subcellular compartments. Amino Acids.
4 Aeschlimann D., Thomazy V. (2000). Protein crosslinking in assembly and remodelling of extracellular matrices: the role of transglutaminases. Connect Tissue Res.
5 McCarthy J.R., Patel P., Botnaru I., Haghayeghi P., Weissleder R., Jaffer F.A. (2009). Multimodal nanoagents for the detection of intravascular thrombi. Bioconjug Chem.
6 Jaffer F.A., Tung C.H., Wykrzykowska J.J., Ho N.H., Houng A.K., Reed G.L., Weissleder R. (2004). Molecular imaging of factor XIIIa activity in thrombosis using a novel, near-infrared fluorescent contrast agent that covalently links to thrombi. Circulation.
7 Mehta K., Kumar A., Kim H.I. (2010). Transglutaminase 2: a multi-tasking protein in the complex circuitry of inflammation and cancer. Biochem Pharmacol.
8 Wilhelmus M.M., van Dam A.M., Drukarch B. (2008). Tissue transglutaminase: a novel pharmacological target in preventing toxic protein aggregation in neurodegenerative diseases. Eur J Pharmacol.
9 Collighan R.J., Griffin M. (2009). Transglutaminase 2 cross-linking of matrix proteins: biological significance and medical applications. Amino Acids.
10 Miserus R.J., Herias M.V., Prinzen L., Lobbes M.B., Van Suylen R.J., Dirksen A., Hackeng T.M., Heemskerk J.W., van Engelshoven J.M., Daemen M.J., van Zandvoort M.A., Heeneman S., Kooi M.E. (2009). Molecular MRI of early thrombus formation using a bimodal alpha2-antiplasmin-based contrast agent. JACC Cardiovasc Imaging.
11 Mazooz G., Mehlman T., Lai T.S., Greenberg C.S., Dewhirst M.W., Neeman M. (2005). Development of magnetic resonance imaging contrast material for in vivo mapping of tissue transglutaminase activity. Cancer Res.
12 Caccamo D., Curro M., Ientile R. (2010). Potential of transglutaminase 2 as a therapeutic target. Expert Opin Ther Targets.